# [^99m^Tc]-Pentavalent dimercaptosuccinic acid

Chemical name: | [^99m^Tc]-Pentavalent dimercaptosuccinic acid
Abbreviated name: | [^99m^Tc]-(V)DMSA
Synonym: | [^99m^Tc]-DMSA
Agent Category: | Compound
Target: | Sodium phosphate co-transporter type III
Target Category: | Transporter
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Humans | Click on the above structure of [^99m^Tc]-DMSA for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Dimercaptosuccinic%20acid&cmd=DetailsSearch)]

Technetium-99m (^99m^Tc)–labeled pentavalent dimercaptosuccinic acid ([^99m^Tc]-(V)DMSA) has been used for renal scintigraphy (see below for references) as well as detection and postoperative evaluation of medullary carcinomas of the thyroid (MCT).[^99m^Tc]-(V)DMSA has been shown to accumulate in breast tumors, head and neck cancers, osteosarcomas, and hepatocellular carcinoma (1). [^99m^Tc]-(V)DMSA has been used for renal (2, 3) and metastatic tumor (4) scintigraphy in animals (2), adults (4), and children (3). The ^99m^Tc in [^99m^Tc]-DMSA has been shown to exist in a trivalent (III) or a pentavalent (V) state, depending on the pH at which the radiolabeled compound was prepared. [^99m^Tc]-(III)DMSA is used as a renal imaging agent, whereas [^99m^Tc]-(V)DMSA is suitable for imaging cancerous tumors (5). Recently, the European Association of Nuclear Medicine revised its guidelines (http://www.eanm.org/scientific_info/guidelines/gl_paed_dmsa_scin.pdf) for the use of [^99m^Tc]-(V)DMSA scintigraphy in children. Also, several clinical trials (http://clinicaltrials.gov/ct2/results?term=dimercaptosuccinic+acid) approved by the United States Food and Drug Administration to evaluate the use of unlabeled DMSA for the treatment of lead exposure, toxicity, and poisoning in children have been completed. The exact mechanism of [^99m^Tc]-(V)DMSA uptake by the tumor cells is not clear, but a report suggests that cellular uptake of this radiotracer is mediated by the sodium phosphate co-transporter type III (NaPi type III) (6).

The biodistribution of [^99m^Tc]-(V)DMSA has been studied in rabbits (7) and mice (8). [^99m^Tc]-(V)DMSA uptake has also been used to the evaluate the efficacy of chemotherapy in patients with multiple myeloma (9) or glioblastoma (10) and to investigate the correlation of breast cancer in women to breast density and expression of the calcitonin gene-related peptide (11).

### Other Sources of Information:

Protein and mRNA (http://www.ncbi.nlm.nih.gov/nuccore/NM_011394.3) sequence of mouse Na-dependent phosphate transporter type II

Chromosome location and gene information (http://www.ncbi.nlm.nih.gov/gene/6569) for human Na-dependent phosphate transporter type II (GeneID: 6567)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc-dimercaptosuccinic%20acid%20synthesis&cmd=DetailsSearch)]

[^99m^Tc]-(V)DMSA is usually synthesized with a freeze-dried kit that is commercially available from several manufacturers (click here for product insert (http://md.gehealthcare.com/shared/pdfs/pi/dmsa.pdf) from a manufacturer), as described by Djokic et al. (12). The kit contains DMSA, stannous chloride, ascorbic acid, sodium chloride, and inositol (as a stabilizer). Reconstitution of the kit in an acidic buffer (pH 2.0–5.0) followed by labeling with ^99m^Tc-pertechnetate was shown to yield primarily [^99m^Tc]-(III)DMSA (71–80% of the total radiochemical product), but labeling closer to the physiological pH (pH 6.5–7.5) or at an alkaline pH (pH 9.0) resulted in the formation of mainly [^99m^Tc]-(V)DMSA (56.0% and 98.0% at pH 6.5 and pH 9.0, respectively) (13). Hirano et al. reported a similar trend of the radiochemical yield for the trivalent and pentavalent [^99m^Tc]-DMSA when synthesized at acidic and alkaline pH levels, respectively (14). A method for the preparation of ultrapure [^99m^Tc]-(V)DMSA (radiochemical purity 100%) has also been published (15). The specific activity of the labeled compound(s) was not reported by any investigator.

Babbar et al. reported that addition of ascorbic acid to the DMSA kit developed for ^99m^Tc labeling increased the shelf-life of the refrigerated kit (6–10°C) from 4 weeks (without ascorbic acid) to 24 weeks (13).

The existence of three isomers (syn-endo, anti, and syn-exo) of [^99m^Tc]-(V)DMSA has been reported by Lam et al. (16). Although [^99m^Tc]-(III)DMSA (Rf = 0–0.1) and [^99m^Tc]-(V)DMSA (Rf = 0.45–0.55) could be separated with thin-layer chromatography (16), separation of the three [^99m^Tc]-(V)DMSA isomers has not been documented. However, the three rhenium 188 (^188^Re)–labeled isomers of DMSA have been isolated with high-performance liquid chromatography by Blower et al. (17).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc-DMSA%20in%20vitro&cmd=DetailsSearch)]

The in vitro binding of [^99m^Tc]-(V)DMSA to rabbit plasma using the trichloro acetic acid precipitation method was reported to be 60% compared with 97% for [^99m^Tc]-(III)DMSA (13). In addition, the blood clearance of [^99m^Tc]-(V)DMSA was observed to be faster than its trivalent analog (13). The fast blood clearance of [^99m^Tc]-(V)DMSA was attributed to its reduced binding to the plasma proteins.

Using three different human cancer cell lines (MCF-7 (origin: breast tumor), G152 (origin: glioblastoma multiforme), and MG-63 (origin: osteosarcoma)), it was demonstrated under in vitro conditions that [^99m^Tc]-(V)DMSA uptake in the cells was facilitated by the NaPi transporter type III (18). In another study using human U937 leukemia cells treated with VP-16 (http://dailymed.nlm.nih.gov/dailymed/drugInfo.cfm?id=4521), a drug that induces apoptosis in cells, increased exposure time to VP-16 reduced accumulation of both phosphate and [^99m^Tc]-(V)DMSA in the apoptotic cells (19).

Investigators have shown that the adsorption of [^99m^Tc]-(V)DMSA to commercially available calcium phosphates and hydroxyapatites (both amorphous and crystalline preparations) under in vitro conditions in presence of 0.1 M phosphate is reversible, is influenced by pH, and does not lead to any dissociation of the complex (16). Under the same test conditions, the adsorption of ^99m^Tc-hydroxymethylene diphosphate to the calcium phosphates and hydroxyapatite preparations remained almost constant. The investigators concluded that the deposition of [^99m^Tc]-(V)DMSA was found only in certain types of bone metastases, which explained why the normal skeleton was not visible clearly in scintigrams of these cancer patients (16).

Le Jeune et al. showed there was a correlation between [^99m^Tc]-(V)DMSA uptake, the phosphatidylinositol-3-kinase (Pi3-K) and protein kinase C (PKC) activities, and the rapid cell proliferation of several malignant glioma cell lines (20). From this study, the investigators suggested that, because Pi3-K and PKC activities have a major role in progression of the glioblastoma, the degree of [^99m^Tc]-(V)DMSA uptake by the malignant glioma cells could be a good indicator of aggressiveness of the cancer.

In a study with cultured Ehrlich ascites tumor cells, Horiuchi et al. showed that the pH of the growth medium influenced the uptake of [^99m^Tc]-(V)DMSA by these cells (21). The investigators showed that the accumulation of radioactivity in these cells was 4.75 ± 0.38% of the dose at a pH range of 8.2–7.4. At pH 7.0, accumulation of radioactivity increased to 9.53 ± 0.94% of the dose; however, at pH 5.3 it increasedto ~22% of the dose.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20rodentia)]

The biodistribution patterns of tetravalent ^99m^Tc-DMSA ([^99m^Tc]-(IV)DMSA) and [^99m^Tc]-(V)DMSA in rats (n = 4 animals/radiocompound) have been described in a technical report from 1985 (22). In this study, a higher amount of [^99m^Tc]-(IV)DMSA (16.4 ± 7.4 percent injected dose per gram tissue (%ID/g)) accumulated in the kidneys of rats compared to [^99m^Tc]-(V)DMSA (1.64 ± 0.22% ID/g). Also, a similar result was obtained when a 1:1 mixture of [^99m^Tc]-(IV)DMSA and [^99m^Tc]-(V)DMSA was injected into the animals, indicating that the tetravalent compound had a specificity to accumulate in the renal organs.

Babbar et al. (13) studied the biodistribution of [^99m^Tc]-(III)DMSA and [^99m^Tc]-(V)DMSA in normal mice (n = 5 animals/radiochemical/time point) given an intravenous injection of the respective labeled compounds. [^99m^Tc]-(III)DMSA was reported to accumulate primarily in the liver (10.71 ± 1.61 and 12.70 ± 0.26% % ID/g at 1 h and 3 h postinjection (p.i.), respectively) and kidneys (18.70 ± 0.61 and 16.31 ± 0.30% ID/g at 1 h and 3 h p.i., respectively), followed by bone (1.91 ± 0.33 and 2.03 ± 0.13% ID/g at 1 h and 3 h p.i., respectively). [^99m^Tc]-(V)DMSA accumulated mainly in the bone (7.83 ± 0.04 and 6.61 ± 0.36% ID/g at 1 h and 3 h p.i., respectively), followed by the kidneys (3.92 ± 0.20 and 2.52 ± 0.10% ID/g at 1 h and 3 h p.i., respectively) and the liver (1.16 ± 0.07 and 0.83 ± 0.02% ID/g at 1 h and 3 h p.i., respectively). A similar uptake profile for the two radiochemicals in mice (n = 5 animals) was reported by Chauhan et al. (8). Also, using [^99m^Tc]-(V)DMSA, these investigators showed that mammary carcinoma tumors in mice could be detected by scintigraphy.

[^99m^Tc]-(V)DMSA was shown to be a better scintigraphic agent than either [^99m^Tc]-(III)DMSA or ^99m^Tc-labeled human immunogammaglobulin for the visualization of inflammation resulting from turpentine-induced abscesses in mice (5).

Small animal single-photon emission computed tomography (SPECT) was performed on mice using [^99m^Tc]-DMSA (isomeric form not reported) and it the tracer was shown to have a spatial resolution of ~1 mm, was suitable to study the renal cortex, and could be used to detect changes in the renal proximal tubule functions in mice (23).

It is well known that cancerous tumors have an acidic environment compared to normal tissues. Therefore, Horiuchi et al. investigated the correlation between [^99m^Tc]-(V)DMSA accumulation in tumor tissue and tissue acidity in mice bearing Ehrlich ascite tumor cells (EATC) (24). Using the double-tracer autoradiography technique with ^14^C-deoxyglucose and [^99m^Tc]-(V)DMSA, the investigators showed there was a correlation between the accumulation of [^99m^Tc]-(V)DMSA in the EATC tumors and the glucose-induced acidification of the tissues (because aerobic glycolysis results in the formation of lactic acid).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc%20%28V%29%20dmsa%20non%20primate%20mammals&cmd=DetailsSearch)]

Watkinson et al. investigated the biodistribution of [^99m^Tc]-(V)DMSA in rabbits with (n = 20 animals) or without (n = 20 animals) transplantable squamous cell carcinoma tumors (7). The investigators reported that both groups of animals showed a similar (P > 0.05) accumulation of the tracer in the kidneys, bone, blood, and the bladder. However, contrary to results obtained by Yokoyama et al. (25), these investigators reported that there was no evidence of [^99m^Tc]-(V)DMSA uptake by the tumors of rabbits in the study. The radiochemical had a bi-exponential clearance from the blood, and the major route of excretion of radioactivity was through the urine.

Ercan et al. reported that glucose acidosis increased the uptake of [^99m^Tc]-(V)DMSA in the bacterial arthritic joints in rabbits with experimental arthritis induced by an intra-articular injection of ovalbumin (5).

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc%28V%29-DMSA%20human%20studies&cmd=DetailsSearch)]

[^99m^Tc]-(V)DMSA scintigraphy was shown by Babbar et al. to detect MCT and metastases of breast carcinoma to the brain in patients (13). Using [^99m^Tc]-(V)DMSA scintigraphy, the detection of MCT in a patient was also reported by Chauhan et al. (8). In another study using SPECT to compare the MCT accumulation of [^99m^Tc]-(V)DMSA, ^131^I-labeled metaiodobenzylguanidine, or ^201^Tl chloride , only [^99m^Tc]-(V)DMSA was shown to detect the tumors (14), therefore confirming the earlier results obtained by Babbar et al. (13) and Chauhan et al. (8).

Basu et al. showed that [^99m^Tc]-(V)DMSA scintigraphy could be used for the detection, diagnosis, and treatment monitoring of skeletal metastases (4). In another study with 10 patients suffering from prostate cancer metastases to the bone, it was shown that [^99m^Tc]-(V)DMSA scans could be used to predict the biodistribution, determine tumoral and renal dosimetry, and assess the suitability of patients for treatment with [^188^Re]-(V)DMSA, a potential therapeutic analog of the scintigraphy agent (26).

In a retrospective study of 24 women with breast cancer who had undergone preoperative scintimammography with [^99m^Tc]-(V)DMSA, it was concluded that the uptake of this tracer was significantly higher (P = 0.001) in cancers expressing the calcitonin gene-related peptide compared with the non-expressing peptide cancers (11). In addition, an increased uptake of [^99m^Tc]-(V)DMSA was particularly apparent in cancers with high breast density containing mixed lesions (i.e., presence of in situ ductal carcinoma along with invasive ductal carcinoma).

Rajic et al. (27) evaluated the use of [^99m^Tc]-(V)DMSA as a marker for renal function in 67 patients suffering from glomerulonephritis, and the investigators concluded that the radiotracer had limited use for precise determination of renal function in these patients. Suzuki et al. (28) used [^99m^Tc]-(V)DMSA to evaluated the renal function of four children suffering from idiopathic tubular proteinuria (also known as Dent disease (http://www.rarekidneystones.org/dent/)) and observed that a low amount of the tracer was retained in the kidney because it was rapidly cleared from the organ into the bladder. On the basis of these results, the investigators suggested that renal scintigraphy with [^99m^Tc]-(V)DMSA could be a useful method to evaluate the renal function of these patients. Similar results were reported by Lee et al. in a recent study with 13 patients (children and adults) having either Dent disease (n = 7 patients) or Lowe syndrome (http://www.ncbi.nlm.nih.gov/bookshelf/br.fcgi?book=gene&part=lowe) (n = 6 patients) (29).

Stathaki et al. evaluated the use of [^99m^Tc]-(V)DMSA and compared the results to scintigraphic results with [^99m^Tc]-labeled hexamethylpropylene amine oxime white blood cell ([^99m^Tc]-HMPAO WBC) for the detection and assessment of inflammatory bowel disease (http://kidshealth.org/parent/medical/digestive/ibd.html) (IBD) in 10 patients (30). From this study, the investigators concluded that [^99m^Tc]-(V)DMSA scintigraphy could be a non-invasive alternative to the use of [^99m^Tc]-HMPAO WBC for the evaluation of IBD in the patients. However, [^99m^Tc]-(V)DMSA scintigraphy was slightly inferior to [^99m^Tc]-HMPAO WBC scintigraphy in determining localization of the disease.

Koutsikos et al. (9) evaluated the use of combined scintigraphy with ^99m^Tc-labeled sestamibi ([^99m^Tc]-sestamibi) and [^99m^Tc]-(V)DMSA to monitor the chemotherapeutic response in 20 patients with multiple myeloma (http://www.cancer.org/docroot/cri/content/cri_2_4_1x_what_is_multiple_myeloma_30.asp) (11 patients evaluated with [^99m^Tc]-sestamibi (group A), and 9 patients in remission with [^99m^Tc]-(V)DMSA (group B)). The number of non-active lesions (NAL) and the total number of uptake-positive lesions (TPL) were determined in the two patient groups as described elsewhere (9), and the NAL/TPL ratios, which represent effectively treated lesions, were calculated. The NAL/TPL ratios were 16:58 for group A and 22:27 for group B, indicating that 27.6% and 81.5% of the lesions were effectively treated in groups A and B, respectively. From this study, the investigators concluded that the NAL/TPL ratios with the two scintigraphy agents could be used to evaluate the chemotherapeutic response in multiple myeloma patients even if a tumor baseline was not available for the patients.

Tsiouris et al. (10) performed a clinical study with a patient suffering from recurrent glioblastoma multiforme (http://www.braintumor.org/Glioblastoma/?gclid=CNeswN6FuaICFRE95Qod-x4H7A) to evaluate the use of [^99m^Tc]-(V)DMSA uptake by the tumor cells as a marker of the proliferative potential of the cancerous tumor. The tumor had been surgically removed from the patient, followed by adjuvant radio- and chemotherapy, but magnetic resonance imaging confirmed recurrence of the cancer a few months later. A second round of chemotherapy did not improve the patient's condition, and [^99m^Tc]-(V)DMSA scintigraphy revealed there was almost no change in proliferation of the tumor after chemotherapy. On the basis of this study, the investigators suggested that scintigraphy with this radiochemical could be used as a non-invasive tumor cell proliferation marker and that this technique may be useful to monitor cancer therapy response(s), predict patient prognosis, and inform patient management.

## Supplemental Information

[Disclaimers]

No supplemental information is currently available.

References
1 Bozkurt M.F., Ugur O., Banti E., Grassetto G., Rubello D. (2008). Functional nuclear medicine imaging of medullary thyroid cancer. Nucl Med Commun.
2 Cabuk M., Gurel A., Sen F., Demircan N. (2008). Renoprotective effect of erdosteine in rats against gentamicin nephrotoxicity: a comparison of 99mTc-DMSA uptake with biochemical studies. Mol Cell Biochem.
3 Yiee, J.H., M. Disandro, M.H. Wang, A. Hittelman, and L.S. Baskin, Does Severity of Renal Scarring on DMSA Scan Predict Abnormalities in Creatinine Clearance? Urology.
4 Basu S., Nair N., Awasare S., Tiwari B.P., Asopa R., Nair C. (2004). 99Tc(m)(V)DMSA scintigraphy in skeletal metastases and superscans arising from various malignancies: diagnosis, treatment monitoring and therapeutic implications. Br J Radiol.
5 Ercan M.T., Gulaldi N.C., Unsal I.S., Aydin M., Peksoy I., Hascelik Z. (1996). Evaluation of Tc-99m(V) DMSA for imaging inflammatory lesions: an experimental study. Ann Nucl Med.
6 Papantoniou V., Tsiouris S., Mainta E., Valotassiou V., Souvatzoglou M., Sotiropoulou M., Nakopoulou L., Lazaris D., Louvrou A., Melissinou M., Tzannetaki A., Pirmettis I., Koutsikos J., Zerva C. (2005). Imaging in situ breast carcinoma (with or without an invasive component) with technetium-99m pentavalent dimercaptosuccinic acid and technetium-99m 2-methoxy isobutyl isonitrile scintimammography. Breast Cancer Res.
7 Watkinson J.C., Allen S.J., Laws D.E., Lazarus C.R., Maisey M.N., Clarke S.E. (1991). The pharmacokinetics and biodistribution of technetium-99m(V)dimercaptosuccinic acid in an animal tumor model. J Nucl Med.
8 Chauhan U.P., Babbar A., Kashyap R., Prakash R. (1992). Evaluation of a DMSA kit for instant preparation of 99mTc(V)-DMSA for tumour and metastasis scintigraphy. Int J Rad Appl Instrum B.
9 Koutsikos J., Athanasoulis T., Anagnostopoulos A., Velidaki A., Passadi M., Dimopoulos M.A., Zerva C. (2005). Combined use of 99mTc-sestamibi and 99mTc-V-DMSA in the assessment of chemotherapy effectiveness in patients with multiple myeloma. J Nucl Med.
10 Tsiouris S., Pirmettis I., Chatzipanagiotou T., Ptohis N., Papantoniou V. (2007). Pentavalent technetium-99m dimercaptosuccinic acid [99m Tc-(V)DMSA] brain scintitomography--a plausible non-invasive depicter of glioblastoma proliferation and therapy response. J Neurooncol.
11 Papantoniou, V., E. Sotiropoulou, P. Valsamaki, A. Tsaroucha, M. Sotiropoulou, N. Ptohis, A. Stipsanelli, K. Dimitrakakis, S. Marinopoulos, S. Tsiouris, and A. Antsaklis, Breast density, scintimammographic (99m)Tc(V)DMSA uptake, and calcitonin gene related peptide (CGRP) expression in mixed invasive ductal associated with extensive in situ ductal carcinoma (IDC + DCIS) and pure invasive ductal carcinoma (IDC): correlation with estrogen receptor (ER) status, proliferation index Ki-67, and histological grade. Breast Cancer.
12 Djokic D., Jankovic D., Nikolic N. (2009). Preparation and in vivo evaluation of 90Y-meso-dimercaptosuccinic acid (90Y-DMSA) for possible therapeutic use: comparison with 99mTc-DMSA. Cancer Biother Radiopharm.
13 Babbar A., Kashyap R., Chauhan U.P. (1991). A convenient method for the preparation of 99mTc-labelled pentavalent DMSA and its evaluation as a tumour imaging agent. J Nucl Biol Med.
14 Hirano T., Tomiyoshi K., Zhang Y.J., Ishida T., Inoue T., Endo K. (1994). Preparation and clinical evaluation of technetium-99m dimercaptosuccinic acid for tumour scintigraphy. Eur J Nucl Med.
15 Kumar V. (2001). Evaluation of stannous oxidation in the preparation of ultrahigh-purity 99m Tc(V)-DMSA. Nucl Med Commun.
16 Lam A.S., Puncher M.R., Blower P.J. (1996). In vitro and in vivo studies with pentavalent technetium-99m dimercaptosuccinic acid. Eur J Nucl Med.
17 Blower P.J., Lam A.S., O'Doherty M.J., Kettle A.G., Coakley A.J., Knapp F.F. (1998). Pentavalent rhenium-188 dimercaptosuccinic acid for targeted radiotherapy: synthesis and preliminary animal and human studies. Eur J Nucl Med.
18 Denoyer D., Perek N., Le Jeune N., Frere D., Dubois F. (2004). Evidence that 99mTc-(V)-DMSA uptake is mediated by NaPi cotransporter type III in tumour cell lines. Eur J Nucl Med Mol Imaging.
19 Denoyer D., Perek N., Jeune N.L., Frere D., Sabido O., Clotagatide A., Dubois F. (2004). In vitro and in vivo evaluation of the influence of type III NaPi co-transporter activity during apoptosis on 99mTc-(V)DMSA uptake in the human leukaemic cell line U937. Eur J Nucl Med Mol Imaging.
20 Le Jeune N., Perek N., Dubois F. (2006). Influence of Pi3-K and PKC activity on 99mTc-(V)-DMSA uptake: correlation with tumour aggressiveness in an in vitro malignant glioblastoma cell line model. Eur J Nucl Med Mol Imaging.
21 Horiuchi K., Saji H., Yokoyama A. (1998). pH sensitive properties of Tc(V)-DMS: analytical and in vitro cellular studies. Nucl Med Biol.
22 Westera G., Gadze A., Horst W. (1985). A convenient method for the preparation of 99mTc(V)dimercaptosuccinic acid (99mTc(V)-DMSA). Int J Appl Radiat Isot.
23 Jouret F., Walrand S., Parreira K.S., Courtoy P.J., Pauwels S., Devuyst O., Jamar F. Single photon emission-computed tomography (SPECT) for functional investigation of the proximal tubule in conscious mice. Am J Physiol Renal Physiol.
24 Horiuchi K., Saji H., Yokoyama A. (1998). Tc(V)-DMS tumor localization mechanism: a pH-sensitive Tc(V)-DMS-enhanced target/nontarget ratio by glucose-mediated acidosis. Nucl Med Biol.
25 Yokoyama A., Hata N., Horiuchi K., Masuda H., Saji H., Ohta H., Yamamoto K., Endo K., Torizuka K. (1985). The design of a pentavalent 99mTc-dimercaptosuccinate complex as a tumor imaging agent. Int J Nucl Med Biol.
26 Blower P.J., Kettle A.G., O'Doherty M.J., Coakley A.J., Knapp F.F. (2000). 99mTc(V)DMSA quantitatively predicts 188Re(V)DMSA distribution in patients with prostate cancer metastatic to bone. Eur J Nucl Med.
27 Rajic M., Bogicevic M., Antic S., Mitic B., Avramovic M., Ilic S., Vlajkovic M., Mitic-Zlatovic M., Stefanovic V. (2002). Alteration of 99mTc-DMSA biodistribution in glomerulonephritis. Nucl Med Rev Cent East Eur.
28 Suzuki S., Suzuki J., Kume K., Yoshida K., Suyama H., Kawasaki Y., Nozawa R., Suzuki H., Fujiki T., Kamiyama S., Suzuki A. (1999). Poor renal accumulation of 99mTc-DMSA in idiopathic tubular proteinuria. Nephron.
29 Lee B.H., Lee S.H., Choi H.J., Kang H.G., Oh S.W., Lee D.S., Ha I.S., Choi Y., Cheong H.I. (2009). Decreased renal uptake of (99m)Tc-DMSA in patients with tubular proteinuria. Pediatr Nephrol.
30 Stathaki M.I., Koutroubakis I.E., Koukouraki S.I., Karmiris K.P., Moschandreas J.A., Kouroumalis E.A., Karkavitsas N.S. (2008). Active inflammatory bowel disease: head-to-head comparison between 99mTc-hexamethylpropylene amine oxime white blood cells and 99mTc(V)-dimercaptosuccinic acid scintigraphy. Nucl Med Commun.